# ^99m^Tc-Labeled 13,13’[oxybis[methylene(2,5-dioxo-1,3-pyrrolidinediyl)]]bis[N-(mercaptoacetyl)-D-tyrosyl-S-(3-aminopropyl)-L-cysteinylglycyl-L-α-aspartyl-L-cysteinylglycylglycyl-S-[(acetylamino)methyl]-L-cysteinylglycyl-S-[(acetylamino)methyl-L-cysteinylglycylglycyl-L-cysteinamide],cyclic(1→5),(1’→5’),-bis(sulfide)

Chemical name: | ^99m^Tc-Labeled 13,13’[oxybis[methylene(2,5-dioxo-1,3-pyrrolidinediyl)]]bis[N-(mercaptoacetyl)-D-tyrosyl-S-(3-aminopropyl)-L-cysteinylglycyl-L-α-aspartyl-L-cysteinylglycylglycyl-S-[(acetylamino)methyl]-L-cysteinylglycyl-S-[(acetylamino)methyl-L-cysteinylglycylglycyl-L-cysteinamide],cyclic(1→5),(1’→5’),-bis(sulfide)
Abbreviated name: | ^99m^Tc-apcitide
Synonym: | ^99m^Tc-P280, ^99m^Tc-peptide 280
Agent Category: | Ligand
Target: | Glycoprotein IIb/IIIa receptor (GPIIb/IIIa receptor)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide)]

Deep vein thrombosis (DVT), which is the formation of blood clots in veins and is also known as venous thromboembolism (VT), is preventable, yet it occurs in the lower extremities of approximately two million Americans each year (1). A majority of DVT patients will experience pulmonary embolism (PE; ~30% are symptomatic, and another 40% are asymptomatic and at high risk) because the blood clot is unstable and can travel to, and lodges in, the lungs. An estimated 100,000 individuals are reported to die every year as a result of PE, and an equal number of people may die from PE-associated conditions such as heart disease and cancer (1). Contrast-enhanced venography is the gold standard for the diagnosis of DVT, but compression ultrasonography is usually the most common technique used to detect VT in the lower extremities. The primary limitation of these procedures is that neither technique can distinguish between chronic and unstable thrombi (2).

Formation of a blood clot is a complex process that requires recruitment of platelets (thrombocytes are cytoplasmic bodies derived from megakaryocytes and have many other functions besides facilitating blood clot formation) for the formation of a thrombus, and the process is described in detail elsewhere (3). One of the important components of the blood clotting process is platelet activation, which leads to the expression of a glycoprotein IIb/IIIa receptor (GPIIb/IIIa receptor) that binds fibrinogen and promotes platelet–platelet interaction, resulting in platelet aggregation and the formation of a secure plug. Several investigators have used radiolabeled monoclonal antibodies targeting fibrin and platelets to identify acute thrombi in humans, but these molecules have limited use because they are cumbersome to manufacture, are large in size, have a long blood circulation time, and present a danger of developing human antibodies directed against mouse antibodies (HAMA) (4). These limitations can be alleviated by the use of synthetic peptides that are much smaller than the monoclonal antibodies, are cleared quickly from circulation, and do not have a potential to produce the HAMA response. In this regard, synthetic peptides containing or mimicking the arginine-glycine-aspartate (RGD) sequence were shown to specifically bind the GPIIb/IIIa receptor, and a radioactive technetium (^99m^Tc)-labeled RGD mimetic peptide, ^99m^Tc-apcitide (^99m^Tc-P280), was shown to selectively accumulate in fresh venous thrombi in dogs (4-6). The study with dogs showed that the thrombus could be detected with scintigraphy 1 h after administration of the radiochemical, and at 4 h the thrombus/muscle ratio was 11 (6). The investigators also studied the biodistribution of ^99m^Tc-apcitide in rats and rabbits. In another study, Muto et al. conducted a preliminary study using ^99m^Tc-apcitide to detect DVT in humans (4). Apcitide is approved (http://www.fda.gov/cder/foi/nda/98/20887.htm) by the United States Food and Drug Administration for the detection and localization of acute VT in humans and is commercially available as a nonradioactive freeze-dried kit (http://www.fda.gov/cder/foi/nda/98/20887_appltrs_prntlbl.pdf) that can be labeled with ^99m^Tc for clinical use (2, 7-9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^99m^Tc-apcitide was described by Lister-James et al. (6). Briefly, a trifluoroacetate salt of P280 was synthesized on a peptide synthesizer using FastMoc™ chemistry on a Rink amide resin. The peptide was purified with preparative reverse-phase (RP) high-performance liquid chromatography (HPLC) on a C_18_ Delta-Pak column. Identification of the P280 peptide was established with amino acid analysis and electrospray mass spectrochemistry. Purity of the peptide was determined to be ≥90% with RP-HPLC as described above.

Labeling of the P280 peptide with ^99m^Tc was also described by Lister-James et al. (6). The P280 peptide was labeled with the use of ^99m^Tc-glucoheptonate, a ligand exchange reagent. The peptide was dissolved in normal saline and mixed with commercially available glucoheptonate previously mixed with ^99m^Tc-sodium pertechnetate. The reaction was allowed to proceed for 15 min at 100°C, and after cooling the solution was sterile-filtered through a low-protein binding 0.22-micron filter. The radiochemical yield and purity were both determined to be ≥90% with instant thin-layer chromatography and HPLC analysis. The specific activity of the labeled product was reported to be ~2,230 GBq/mmol (~60 Ci/mmol) P280 peptide.

The commercially available freeze-dried kit has been described in the draft package insert (http://www.fda.gov/cder/foi/nda/98/20887_appltrs_prntlbl.pdf) of nonradioactive apcitide. Each vial of the kit contains bibapcitide (a dimer of apcitide), sodium glucoheptonate dihydride, stannous chloride dihydride, and sufficient sodium hydroxide or hydrochloric acid to adjust the pH to 7.4 before freeze-drying. The freeze-dried powder, containing no preservative, is then sealed with a rubber stopper under a nitrogen atmosphere. The peptide was labeled with ^99m^Tc as described above, and the specific activity of the labeled product was calculated to be 11.2–33.6 MBq/μM (303–909 μCi/μM) depending on final volume (1–3 mL) of the labeled product (7). ^99m^Tc-Apcitide was used within 6 h of labeling.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide+in+vitro)]

Lister-James et al. (6) determined the 50% inhibition concentration (IC_50_) of P280 for human platelet aggregation using inhibition curves as described by Zucker (10). A fixed number of the platelets were respectively exposed to varying concentrations of the peptide to obtain curves representing percent platelet aggregation versus peptide concentration. The IC_50_ of P280 for platelet aggregation was determined from the curves to be 0.079 ± 0.017 μM. The investigators also compared the inhibition platelet aggregation by P280 in dogs and humans (6). The IC_50_ for dog platelets was reported to be 0.20 ± 0.11 μM compared with 0.056 ± 0.011 μM for the human platelets. This showed that the peptide was 2.5–3.5 times more potent in inhibiting human platelet aggregation than dog platelet aggregation.

In another in vitro assay described elsewhere (11, 12), P280 was shown to inhibit the binding of fibrinogen to the GPIIb/IIIa receptor with an IC_50_ of 6.8 nM (6). Under the same conditions, the IC_50_ of P280 to inhibit the binding of vitronectin to the vitronectin receptor was 12,900 nM, indicating that the P280 peptide was three logs more selective for the GPIIb/IIIa than the vitronectin receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide+rodentia)]

Lister-James et al. studied the biodistribution of ^99m^Tc-apcitide in normal Sprague-Dawley rats (6). The animals were injected with ^99m^Tc-apcitide through the tail vein and euthanized (n = 3/group) at 5, 30, 60, and 120 min after injection. Blood and tissue samples were obtained from the animals, and accumulated radioactivity was counted after washing (tissue only) with normal saline. The radioactivity was reported to be rapidly cleared from circulation over 2 h, and 70% of the radioactivity was cleared from the tissue during this time. Little radiotracer was observed to accumulate in the gastrointestinal tract and the other tissues. Radioactivity was excreted primarily through the kidneys. No competition studies using unlabeled P280 were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide+rodentia+non+primate+mammals)]

Lister-James et al. performed imaging studies in mongrel dogs after creating a thrombus in one of the hind leg femoral veins of the animals (6). The other femoral vein was used as a control. Six dogs were injected with ^99m^Tc-apcitide as a bolus in the foreleg through the intravenous route. Three dogs were used as positive controls and injected with ^99m^Tc-hexamethylpropyleneamine oxime (HMPAO)-labeled autologous platelets (^99m^Tc-HMPAO platelets) as described by Becker et al. (13). Two dogs were injected with ^99m^Tc-glucoheptonate as negative controls. Images of the hind legs (with a lead shield placed over the bladder) were acquired at 12 min and ~1, 2, 3, and 4 h after the injection. From the images with ^99m^Tc-apcitide it was evident that the thrombus was visible after 13 min after injection. The thrombus was not visible with ^99m^Tc-glucoheptonate even 2 h after administration of radioactivity, but the dogs treated with ^99m^Tc-HMPAO platelets had very clear images of the thrombus 2 h after treatment. However, the labeled platelets are not the preferred method to visualize thrombi because they require a great deal of manipulation to radiolabel ex vivo and have slow pharmacokinetics (14).

A region of interest analysis of the various images obtained with the ^99m^Tc-apcitide treatment of the dogs showed rapid blood clearance of the radioactivity, and the label was excreted primarily through the liver and kidneys (6). The amount of ^99m^Tc-apcitide accumulated in the thrombi was 0.0059% of the injected dose/gram of tissue (% ID/g), and the vessels containing the thrombi had a radioactivity accumulation of 0.0040% ID/g (6). The thrombus/blood (T/B) and thrombus/muscle (T/M) ratios 4 h after treatment were reported to be 4.4 ± 0.74 and 11 ± 7.0, respectively. During the same time, the T/B and T/M ratios for the control dogs was reported to be 2.2 ± 0.8 and 4.3 ± 2.4, respectively. For the positive control animals, which were treated with the labeled platelets, the T/B and T/M ratios were 5.4 ± 3.2 and 230 ± 100.0, respectively.

Lister-James et al. also studied the biodistribution of ^99m^Tc-apcitide in New Zealand white rabbits (6). The animals were injected with the labeled peptide through the ear vein, and the animals were euthanized 5, 30, 60, 120, and 240 min after injection. Blood and various organs (after washing with saline and blotting dry) were collected from the animals, and accumulated radioactivity was counted . The radioactivity was reported to clear rapidly from blood within 4 h after injection. Some radioactivity accumulated in the bile and the colon, but clearance of radioactivity through the gastrointestinal tract was not clearly apparent. Approximately 70% of the radioactivity was reported to be cleared through the urinary route.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+apcitide+human+studies)]

Muto et al. reported the use of ^99m^Tc-apcitide imaging to detect DVT in nine patients (4). No adverse effects on the patients were reported, and the thrombi were visible in eight of the nine patients 1 h after treatment with the radiochemical. All the positive cases had an onset of DVT in <3 weeks, and the only negative case was diagnosed ~6 weeks earlier. PE was detected in two patients, and a third patient showed an accumulation of ^99m^Tc-apcitide in a hemagioblastoma. From these results the investigators concluded that the use of ^99m^Tc-apcitide scintigraphy is a safe and sensitive procedure for the diagnosis of DVT and PE.

Two preliminary reports detailing the use of ^99m^Tc-apcitide for DVT imaging in clinical trials of humans are available (9, 15). A detailed account of two clinical trials comparing the use of ^99m^Tc-apcitide with contrast venography for the imaging of DVT was later published by Taillefer et al. (16). Two hundred eighty patients either showing signs and symptoms of acute DVT or having a high risk of DVT after surgery were reported to be enrolled in the two clinical trials. Imaging with ^99m^Tc-apcitide and contrast venography was performed on the patients within 36 h of enrollment. Only 243 patients participating in the trials were evaluable. Compared with contrast venography, ^99m^Tc-apcitide scintigraphy had a sensitivity, specificity, and agreement of 73.4%, 67.5%, and 69.1%, respectively. In one of the institutions involved in the clinical trial, data obtained from a subset of patients (n = 63), who had no history of acute DVT or PE and presented at the institute within 3 days of the onset of DVT symptoms, showed that ^99m^Tc-apcitide scintigraphy compared with contrast venography had a sensitivity, specificity, and agreement of 90.6%, 83.9%, and 87.3%, respectively. On the basis of this information the investigators concluded that ^99m^Tc-apcitide scintigraphy is a new, sensitive modality that could be used for imaging acute DVT.

Bates et al. (7) evaluated the use of ^99m^Tc-apcitide for the detection of recurrent DVT in 78 patients. Of these, 38 patients were newly diagnosed with DVT (group 1), and 40 patients were previously diagnosed (group 2) with DVT and showed postthrombotic symptoms. The investigators expected that scintigraphy with ^99m^Tc-apcitide would be positive only in individuals with the acute (recent) condition because GPIIb/IIIa is expressed only on activated platelets that participate in the formation of the thrombus. Patients with old, inactive thrombi were expected to be negative for DVT with this technique. The images were interpreted by two expert nuclear medicine physicians in a blinded fashion. The sensitivity and specificity of ^99m^Tc-apcitide were respectively based on the proportion of group 1 patients who were positive for acute DVT and the proportion of group 2 individuals who were negative for the condition. On the basis of the results of the two experts, who had excellent agreement on interpretation of the images, it was concluded that ^99m^Tc-apcitide has a sensitivity of 92% and a specificity of 82%. The investigators concluded that ^99m^Tc-apcitide scintigraphy could be used to detect acute DVT and has few false positive results in patients having a previous history of DVT. However, accuracy of the interpretation was dependent on the training and experience of the interpreting physicians.

Dunzinger et al. investigated the use of ^99m^Tc-apcitide for the detection of DVT and PE in 19 patients (2). The patients received the radiochemical through an intravenous injection within 24 h of presentation at the hospital. Scintigraphic images were compared with results obtained from ultrasonography and/or contrast venography, and patients suspected to have PE underwent computed tomography or lung perfusion scans. Scintigraphy was reported to detect acute DVT in 14 of 16 patients diagnosed with the condition using the other modalities. In the 14 DVT-positive patients, the thrombi were visible with scintigraphy up to 17 days after the clinical symptoms were apparent. Three patients without DVT, as determined with other modalities, were reported to be negative even with scintigraphy. Only 1 of 6 patients with PE was positive on the basis of scintigraphy. From these results the investigators concluded that ^99m^Tc-apcitide scintigraphy had a sensitivity and specificity of 87% and 100%, respectively, for patients with DVT. However, ^99m^Tc-apcitide scintigraphy did not detect PE in 83% of the patients.

## References

1 Rahman, S., Deep Vein Thrombosis Prophylaxis: Friend or Foe. Am J Ther, 2008
2 Dunzinger A., Hafner F., Schaffler G., Piswanger-Soelkner J.C., Brodmann M., Lipp R.W. (2008). (99m)Tc-apcitide scintigraphy in patients with clinically suspected deep venous thrombosis and pulmonary embolism. Eur J Nucl Med Mol Imaging.
3 Furie B., Furie B.C. (2008). Mechanisms of thrombus formation. N Engl J Med.
4 Muto P., Lastoria S., Varrella P., Vergara E., Salvatore M., Morgano G., Lister-James J., Bernardy J.D., Dean R.T., Wencker D., et al. (1995). Detecting deep venous thrombosis with technetium-99m-labeled synthetic peptide P280. J Nucl Med.
5 Weisel J.W., Nagaswami C., Vilaire G., Bennett J.S. (1992). Examination of the platelet membrane glycoprotein IIb-IIIa complex and its interaction with fibrinogen and other ligands by electron microscopy. J Biol Chem.
6 Lister-James J., Knight L.C., Maurer A.H., Bush L.R., Moyer B.R., Dean R.T. (1996). Thrombus imaging with a technetium-99m-labeled activated platelet receptor-binding peptide. J Nucl Med.
7 Bates S.M., Lister-James J., Julian J.A., Taillefer R., Moyer B.R., Ginsberg J.S. (2003). Imaging characteristics of a novel technetium Tc 99m-labeled platelet glycoprotein IIb/IIIa receptor antagonist in patients With acute deep vein thrombosis or a history of deep vein thrombosis. Arch Intern Med.
8 Reinisch J.F., Bresnick S.D., Walker J.W., Rosso R.F. (2001). Deep venous thrombosis and pulmonary embolus after face lift: a study of incidence and prophylaxis. Plast Reconstr Surg.
9 Taillefer R., Therasse E., Turpin S., Lambert R., Robillard P., Soulez G. (1999). Comparison of early and delayed scintigraphy with 99mTc-apcitide and correlation with contrast-enhanced venography in detection of acute deep vein thrombosis. J Nucl Med.
10 Zucker M.B. (1989). Platelet aggregation measured by the photometric method. Methods Enzymol.
11 Barker P.L., Bullens S., Bunting S., Burdick D.J., Chan K.S., Deisher T., Eigenbrot C., Gadek T.R., Gantzos R., Lipari M.T., et al. (1992). Cyclic RGD peptide analogues as antiplatelet antithrombotics. J Med Chem.
12 Burnier, J.P., T. Gadek, and R. McDowell, Platelet aggregation inhibitors having high specificity for GPIIb/IIIa., in WO 92/17492, I.P.A. Publication, Editor. 1992, Geneva, Switzerland
13 Becker W., Borner W., Borst U. (1988). 99Tcm hexamethylpropyleneamineoxime (HMPAO) as a platelet label: evaluation of labelling parameters and first in vivo results. Nucl Med Commun.
14 Knight L.C. (1990). Radiopharmaceuticals for thrombus detection. Semin Nucl Med.
15 Carretta R.F., Streek P.V., Weiland F.L. (1999). Optimizing images of acute deep-vein thrombosis using technetium-99m-apcitide. J Nucl Med Technol.
16 Taillefer R., Edell S., Innes G., Lister-James J. (2000). Acute thromboscintigraphy with (99m)Tc-apcitide: results of the phase 3 multicenter clinical trial comparing 99mTc-apcitide scintigraphy with contrast venography for imaging acute DVT. Multicenter Trial Investigators. J Nucl Med.